# Lys-cys-cys-tyr-ser-leu-(gly-ser-gly)-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-^111^In

Chemical name: | Lys-cys-cys-tyr-ser-leu-(gly-ser-gly)-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-^111^In
Abbreviated name: | ^111^In-DOTA-(GSG)-KCCYSL
Synonym:
Agent Category: | Peptide
Target: | ErbB-2 extracellular domain
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | .

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+)]

The epidermal growth factor (EGF) and its receptor (EGFR) are known to play a role in the neoplastic transformation of cells (1). The EGFR is a tyrosine kinase receptor family that includes four members, EGFR and three other human EGF receptors (HERs) designated as HER2/ErbB2, HER3/ErbB3, and HER4/ErbB4. The four receptors constitute the HER-kinase axis and regulate cellular responses through complex receptor–ligand interactions. The various signal transduction pathways that respond to EGFR activation and mediate cell responses have been described by Brandt et al. (2). The various EGFRs are known to be amplified, mutated, or overexpressed in several cancers and are a target for the development of pharmaceutical agents that inhibit either the receptor or the signal transduction pathway (3). It has also been reported that the detection of circulating ErbB2-positive tumor cells indicates a poor prognosis for the cancer patient (4). A variety of inhibitors, including small molecules, antibodies, vaccines, and gene therapies, have been developed and tested against the EGFRs for the treatment of cancer (5, 6). However, to achieve therapeutic effects the receptor or signal transduction pathway must be involved in maintenance of the malignant phenotype because HER inhibitor therapy does not necessarily result in treatment of a cancer (7).

The use of antibodies alone against EGFR (e.g., cetuximab) and ErbB2 (e.g., trastuzumab) for the treatment of cancer has yielded only moderate results, and it has been observed that antibodies are most useful when used in combination with chemotherapy (8). In some cases cardiotoxicity has been reported in individuals treated with trastuzumab in combination with some chemotherapeutic agents (9). In an effort to develop better and safer anti-cancer drugs, investigators have attempted to use peptides that bind to receptors on tumors to treat the disease (10, 11). The development of peptide pharmaceuticals has also been pursued because, compared to the larger biomolecules such as antibodies, these molecules are easier to synthesize and have low immunogenicity, rapid blood clearance, and a higher uptake in tumor tissue (12). Using bacteriophage technology, a peptide of six amino acids, lys-cys-cys-tyr-ser-leu (KCCYSL), that specifically recognizes and binds the extracellular domain of ErbB2 was identified, and the investigators hypothesized that the peptide could be developed into an imaging and therapeutic agent against cancer cells that overexpress ErbB2 (13). As an extension to the earlier study, the tumor imaging and targeting ability of KCCYSL was evaluated after labeling with radioactive indium (^111^In). Using the labeled peptide, Kumar et al. performed in vitro and in vivo studies in human breast carcinoma cells that overexpress ErbB2 and in xenografted mice (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+synthesis)]

The procedure used to identify and characterize KCCYSL from a phage display library as an ErbB2 extracellular domain binding peptide was described in detail by Karasseva et al. (13). The synthesis of ^111^In-labeled KCCYSL was described by Kumar et al. (14). The peptide was synthesized using solid-phase Fmoc technology on a peptide synthesizer. The bifunctional chelator 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) was linked with KCCYSL through a gly-ser-gly (GSG) spacer placed between the amino terminus of DOTA and the hexapeptide to obtain DOTA-(GSG)-KCCYSL. For use as control, a scrambled peptide version (KYLCSC) was also prepared similarly. The peptides were purified by reverse-phase high-pressure liquid chromatography (RP-HPLC) on a Vydac C_18_ column. The peptides were freeze-dried and stored at -20°C until required. Electrospray ionization-mass spectrometery was used to confirm the identity of the peptides. Details of how this technique was used to confirm the identity of the peptides were not provided in the publication.

For radiolabeling, the respective peptides were mixed with radioactive [^111^In]indium chloride in ammonium acetate buffer (pH 5.5) (14). The mixture was incubated at 85°C for 60 min, and the reaction was terminated by the addition of ethylenediamine tetraacetic acid to remove unreacted ^111^In. The labeled conjugates were then purified by RP-HPLC and flush-dried with nitrogen gas, and the pH was adjusted to 8.0 with sodium phosphate buffer in saline. Tris(2-carboxyethyl)phosphine hydrochloride was then added to the peptide stock solution to prevent oxidation of the cysteine thiols. Although the radiolabeling efficiency of the reaction was reported to be 40–50%, the specific activity, radiochemical yield, and purity of the product was not provided by the investigators (14). The labeled peptide was reported to be stable for 12 h in phosphate-buffered saline and for at least 1 h in mouse serum.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+in+vitro)]

The in vitro binding of ^111^In-DOTA(GSG)-KCCYSL was investigated in MDA-MB-435 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=HTB-129) cells that express ErbB2 receptors (14). For the same study, K-562 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CCL-243) cells, which do not express ErbB2 receptors, were used as negative controls. The cells were incubated with the radiolabeled peptide for various times at 37°C, and binding of the label with MDA-MB-435 cells increased gradually and reached saturation by 2 h. Under the same conditions the K-562 cells bound little radioactivity. Neither cell line bound the scrambled version of the labeled peptide. In competition experiments with MDA-MB-435 cells, using an increasing concentration of cold DOTA(GSG)-KCCYSL, the binding of radioactivity decreased in a concentration-dependent manner, indicating a specificity of the labeled peptide for ErbB2 receptors (14). The 50% inhibitory concentration of the labeled peptide with these cells was determined to be 42.5 ± 2.67 nM.

To determine internalization of bound radioactivity, the MDA-MB-435 cells were incubated with the labeled peptide for different time periods and washed with ice-cold cell-binding medium to remove any unbound radioactivity. The cells were then incubated on ice with acetic acid in saline for 5 min and pelleted by centrifugation. Radioactivity was counted to determine the internalized (cell pellet) and the surface bound fraction (supernatant). The cell surface–associated label increased up to 2 h and ~11% of the total radioactivity was determined to be internalized during this period (P < 0.0001).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+rodentia)]

The biodistribution of ^111^In-DOTA(GSG)-KCCYSL was investigated in severe combined immunodeficient mice that had MDA-MB-435 cells implanted in the shoulder (14). The radioactive peptide was injected into the mice through the tail vein, and the animals were euthanized in groups of three at different time points. The tissues of interest were collected and counted for incorporated radioactivity, and the uptake was expressed as a percentage of the injected radioactivity dose per gram (% ID/g). Distribution of the radiolabeled peptide was determined at various time points between 15 min and 24 h after administration (14). The tumor uptake of radioactivity decreased from 2.12 ± 0.32% ID/g at 30 min to 0.66 ± 0.11% ID/g at 2 h and to 0.33 ± 0.05% ID/g at 4 h. The blood radioactivity level was 3.16 ± 0.33% ID/g at 15 min after the injection and dropped to 0.13 ± 0.03% ID/g at 2 h. This indicated a rapid uptake of radioactivity by the tumor and a clearance from the blood during the same period. The tumor/blood ratio was 5.0 at the end of 2 h. A radioactivity peak of 10.51 ± 0.07% ID/g was observed in the kidneys at 15 min, and this subsequently decreased to 5–7% ID/g for the next 3 h after injection. This was probably because the radioactive peptide and its breakdown products were excreted primarily through the urinary route. A high level of radioactivity (3.18 ± 0.16% ID/g) was also detected in the lungs at 15 min after the injection, but this level decreased to 0.23 ± 0.17% ID/g at 4 h. The investigators suggested that the lungs showed a high amount of radioactivity probably because these organs are highly vascularized and have a high blood perfusion rate. During the same period, little radioactivity was observed in the other vital organs, muscle, or bone (14).

The specificity of tumor radioactivity uptake was evaluated by performing a competition experiment using unlabeled In-DOTA(GSG)-KCCYSL (14). The mice (n = 3) were injected with the unlabeled peptide (~0.07 μM) through the tail vein followed by administration of the labeled homolog 15 min later. The labeled peptide alone was administered to another group of mice (n = 3) to serve as the positive control. Results indicated that uptake of the radioactive peptide was blocked by 50% in tumors of mice injected with the non-radioactive peptide (P = 0.0012). Administration of the non-labeled peptide did not affect the percentage of radioactivity uptake per gram of tissue in the normal organs, including the kidneys and the lungs, of these animals (14). The investigators suggested that these observations indicate that uptake of the radiolabeled peptide by the tumor was receptor-mediated, but the label observed in the kidneys and the lungs was the result of non-specific uptake of the peptide (14).

In vivo single-photon emission computed tomography of mice injected with ^111^In-DOTA(GSG)-KCCYSL showed that the radioactivity accumulated mainly in the xenografted human breast carcinoma cell tumors and the kidneys (14). Very low radioactivity was detected in the hepatobiliary or other systems of the animals. From these results the investigators concluded that ^111^In-DOTA(GSG)-KCCYSL was a promising peptide for the imaging of ErbB2-positive tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+Non+primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ErbB2+binding+radiolabeled+peptide+Humans)]

No references are currently available.

## NIH Support

The imaging study reported in this chapter was funded by an NIH P50 Grant #CA103130.

## References

1 Gross M.E. Shazer R.L. Agus D.B. Targeting the HER-kinase axis in cancer Semin Oncol 2004 31Suppl 31 9 20 15052539
2 Brandt B., Meyer-Staeckling S., Schmidt H., Agelopoulos K., Buerger H. (2006). Mechanisms of egfr gene transcription modulation: relationship to cancer risk and therapy response. Clin Cancer Res.
3 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
4 Wulfing P., Borchard J., Buerger H., Heidl S., Zanker K.S., Kiesel L., Brandt B. (2006). HER2-positive circulating tumor cells indicate poor clinical outcome in stage I to III breast cancer patients. Clin Cancer Res.
5 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
6 Hudis C.A. (2007). Trastuzumab--mechanism of action and use in clinical practice. N Engl J Med.
7 Bates S.E., Fojo T. (2005). Epidermal growth factor receptor inhibitors: a moving target?. Clin Cancer Res.
8 Khalil M.Y., Grandis J.R., Shin D.M. (2003). Targeting epidermal growth factor receptor: novel therapeutics in the management of cancer. Expert Rev Anticancer Ther.
9 Seidman A., Hudis C., Pierri M.K., Shak S., Paton V., Ashby M., Murphy M., Stewart S.J., Keefe D. (2002). Cardiac dysfunction in the trastuzumab clinical trials experience. J Clin Oncol.
10 Abraham J.M., Sato F., Cheng Y., Paun B., Kan T., Olaru A., Jin Z., Yang J., Agarwal R., David S., Hamilton J.P., Ito T., Mori Y., Meltzer S.J. (2007). Novel Decapeptides that Bind Avidly and Deliver Radioisotope to Colon Cancer Cells. PLoS ONE.
11 Nava-Parada P., Emens L.A. (2007). GV-1001, an injectable telomerase peptide vaccine for the treatment of solid cancers. Curr Opin Mol Ther.
12 Landon L.A., Zou J., Deutscher S.L. (2004). Is phage display technology on target for developing peptide-based cancer drugs?. Curr Drug Discov Technol.
13 Karasseva N.G., Glinsky V.V., Chen N.X., Komatireddy R., Quinn T.P. (2002). Identification and characterization of peptides that bind human ErbB-2 selected from a bacteriophage display library. J Protein Chem.
14 Kumar S.R., Quinn T.P., Deutscher S.L. (2007). Evaluation of an 111In-Radiolabeled Peptide as a Targeting and Imaging Agent for ErbB-2 Receptor Expressing Breast Carcinomas. Clin Cancer Res.